# N-Alkyl-polyethylenimine 2 kDa–stabilized superparamagnetic iron oxide nanoparticles for MRI cell tracking

Chemical name: | N-Alkyl-polyethylenimine 2 kDa–stabilized superparamagnetic iron oxide nanoparticles for MRI cell tracking
Abbreviated name: | Alkyl-PEI2k/SPIO
Synonym: | N-alkyl-PEI2k/SPIO, Alkyl-PEI/SPIO
Agent Category: | Nanoparticles
Target: | Others (mesenchymal stem cell labeling)
Target Category: | Non-targeted
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Superparamagnetic iron oxide (SPIO)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=cell+tracking+and+MRI)]

N-Alkyl-polyethylenimine 2 kDa (PEI2k)–stabilized superparamagnetic iron oxide (SPIO) nanoparticles, abbreviated as alkyl-PEI2k/SPIO, is a contrast agent that was synthesized by Liu et al. for stem cell labeling and tracking with magnetic resonance imaging (MRI) (1).

MRI of SPIO-labeled stem cells has been considered to be the best choice for in vivo cell tracking because of its ability to follow the labeled cells for months as well as to provide detailed anatomic information with high resolution and soft tissue contrast (2, 3). Cells are labeled in situ by direct injection of the SPIO-based agents into the tissue area of interest; cells are labeled in vivo by intravenous administration of the agents (4, 5). In both preclinical and clinical situations, cells are typically labeled in vitro for cell-tracking studies (4). Generally, SPIO nanoparticles need to be coated with organic polymers or other materials for efficient cell labeling. This surface coating increases the stability of SPIO nanoparticles and allows further chemical modifications with ligands (1, 4). In addition, the surface coating could influence the SPIO distribution within cells, which would thus influence the T2 relaxivity. However, there are still a lot of challenges to turn MRI cell tracking into a robust technique either in preclinical settings or in clinical applications. For example, it is impossible to discriminate live cells from dead cells, and to differentiate transplanted cells from macrophages. MRI quantification of both iron oxide concentration and cell number is also not reliable.

It has been shown that SPIO particles clustered in dense vacuoles yield better local contrast enhancement than SPIO particles distributed in cytoplasm (1, 6). Controlled clustered SPIO nanoparticles can greatly shorten T2 relaxation time in comparison with single SPIO nanoparticles at the same iron concentration (1, 6). N-Alkyl-polyethylenimine 25 kDa (PEI25k) is a commercial reagent used for gene transfection. Wang et al. applied PEI25k to stabilize SPIO, and the generated nanoparticles exhibited a controlled clustering structure, efficient cell uptake, and high T2 relaxivity when they were used to label mesenchymal stem cells (MSCs) (6). However, PEI25k has been found to be toxic to labeled cells, resulting in cell death, apoptosis, and differentiation inhibition. In comparison, lower molecular weight PEI, such as PEI2k, is more biocompatible. Liu et al. applied PEI2k to form stable nanocomplexes with SPIO (1). The generated nanoparticles, alkyl-PEI2k/SPIO, could hold multiple SPIO particles with a controlled clustering structure. Labeled MSCs showed no evident toxic effect on their viability, proliferation, and differentiation capacity.

### Related Resource Links:

- Chapters on cell tracking in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=cell+tracking+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)
- Clinical trials for cell tracking in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=cell+tracking+and+imaging)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20869767)]

Liu et al. described the synthesis of alkyl-PEI2k/SPIO in detail (1). Branched PEI2k was reacted with 1-iodododecane in ethanol to generate alkylated PEI2k, which was confirmed with ^1^H nuclear magnetic resonance with ~11% dodecyl substitution. The SPIO nanoparticles dispersed in chloroform were then mixed with alkylated PEI2k at different polymer/SPIO mass ratios to generate alkyl-PEI2k/SPIO. The alkyl-PEI2k/SPIO nanoparticles were characterized with dynamic light scattering (DLS), zeta potential, atomic force microscopy (AFM), and transmission electron microscopy. T2 relaxivity was measured at room temperature with 3 T and spin-echo sequence (TR = 5,000 ms, TE = 10–500 ms).

The alkyl-PEI2k/SPIO nanoparticles displayed positive charges at ~40 mV, which was not significantly affected by the PEI2k polymer/SPIO mass ratios and the micelle size. The T2 relaxivity values were 345, 121, and 84 Fe mM−^1^s−^1^ for the nanoparticles synthesized at polymer/SPIO ratios of 0.6, 1.2, and 2.5, respectively. At the polymer/SPIO mass ratio of 0.6, the generated alkyl-PEI2k/SPIO nanoparticles were well dispersed without obvious aggregation and each nanoparticle was composed of a cluster of a few closely-packed SPIO particles. The diameters of the alkyl-PEI2k/SPIO nanoparticles were 54.7 ± 9.5 and 65 ± 17.2 nm as determined with DLS and AFM, respectively. The sensitivity limit was ~2 µg Fe/ml, which is defined as the alkyl-PEI2k/SPIO concentration at which MRI signal intensity decreases to 50% of that for pure water in T2-weighted images. The alkyl-PEI2k/SPIO nanoparticles with the N-alkyl-PEI2k/SPIO mass ratio of 0.6 were selected by Liu et al. for further testing because of the lower PEI requirement and controlled clustering of SPIO nanoparticles with high T2 relaxivity and stability (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20869767)]

MSCs were labeled with alkyl-PEI2k/SPIO for cell tracking studies (1). MSCs were collected from femurs of male Balb/C mice (18–20 g) and were cultured for three to five passages before use. MSCs were incubated with alkyl-PEI2k/SPIO at different concentrations (0.5, 1, 3.5, and 7 µg Fe/ml) for different incubation periods (1, 6, and 24 h). Cells without exposure to alkyl-PEI2k/SPIO were used as controls.

The SPIO uptake in MSCs was time- and dose-dependent. Prussian blue staining showed that nearly 100% of the MSCs were labeled at a concentration of 7 µg Fe/ml for 24 h incubation, which was further confirmed with flow cytometry (93 ± 2%). Cells labeled with a concentration of 0.5 µg Fe/ml for 24 h had iron content similar to that observed at a concentration of 7 µg Fe/ml after 1 h incubation (P > 0.05). The uptake quantities sufficient for cellular MRI (>2 pg Fe/cell) were achieved when labeling at a concentration of 1 µg Fe/ml for 24 h and the cellular iron content increased to 7.1 pg/cell in MSCs treated with 7 µg Fe/ml for 24 h incubation.

Cells incubated with 0.5, 1, 3.5, and 7 µg Fe/ml exhibited viability comparable to that of unlabeled control cells based on cell viability assays. There was no obvious morphological difference between labeled and unlabeled cells. No significant apoptosis was induced by SPIO labeling. The alkyl-PEI2k/SPIO nanoparticles were observed in the intracellular space, not in the cell nuclei.

The alkaline phosphatase activity of the labeled cells was 32.5 ± 1.8 U/l, similar to that of the control cells (34.4 ± 1.9 U/l) (P > 0.05), indicating that the labeling didn’t compromise the function of osteogenic differentiation, which was also demonstrated with alizarin red staining. The chondrogenic differentiation capability was also unaffected by SPIO labeling as indicated by the staining of proteoglycan-rich extracellular matrix with safranin O and toluidine blue. SPIO labeling led to a significant decrease of the transferrin receptor (TfR) mRNA expression in labeled MSCs as early as 1 d after labeling compared with unlabeled MSCs. A slight recovery of the TfR expression was then observed after the first passage (3 days after labeling), possibly due to feedback of the intracellular iron. For ferritin, after treatment with indicated concentrations of SPIO for 1 d or 3 d, an increasing trend was observed in its mRNA level, which was significantly higher in labeled MSCs than in control cells. Downregulation of TfR and upregulation of ferritin in labeled cells may protect cells from possible cytotoxicity induced by higher intracellular iron concentrations (1, 7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20869767)]

Labeled and unlabeled MSCs in collagen hydrogels were separately injected subcutaneously into the flank of mice and monitored for 19 days with MRI (1). T2-Weighted MRI showed that the labeled MSCs were visible as a hypointense area with sharp borders at the injection site. T2 values decreased from 163 ms to 46 ms as the number of cells increased (10^4^–10^6^). The signal intensity ratios of the control/labeled cells were 30.1, 15.3, 11.7, and 8.9 on days 1, 3, 7, and 19 after injection, respectively. The hypointensity of the labeled MSCs remained visible for at least 19 days. Ex vivo hematoxylin and eosin staining of the cells demonstrated that both labeled and unlabeled cells were alive 19 days after implantation. Prussian blue staining showed that a large number of blue-positive cells were viable at the injection site. These results indicate that the hypointense MRI images were induced by SPIO labeling.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Liu G., Wang Z., Lu J., Xia C., Gao F., Gong Q., Song B., Zhao X., Shuai X., Chen X., Ai H., Gu Z. (2011). Low molecular weight alkyl-polycation wrapped magnetite nanoparticle clusters as MRI probes for stem cell labeling and in vivo imaging. Biomaterials.
2 Arbab A.S., Liu W., Frank J.A. (2006). Cellular magnetic resonance imaging: current status and future prospects. Expert Rev Med Devices.
3 Bulte J.W. (2009). In vivo MRI cell tracking: clinical studies. AJR Am J Roentgenol.
4 Himmelreich U., Dresselaers T. (2009). Cell labeling and tracking for experimental models using magnetic resonance imaging. Methods.
5 Srinivas M., Aarntzen E.H., Bulte J.W., Oyen W.J., Heerschap A., de Vries I.J., Figdor C.G. (2010). Imaging of cellular therapies. Adv Drug Deliv Rev.
6 Wang Z., Liu G., Sun J., Wu B., Gong Q., Song B., Ai H., Gu Z. (2009). Self-assembly of magnetite nanocrystals with amphiphilic polyethylenimine: structures and applications in magnetic resonance imaging. J Nanosci Nanotechnol.
7 Pawelczyk E., Arbab A.S., Pandit S., Hu E., Frank J.A. (2006). Expression of transferrin receptor and ferritin following ferumoxides-protamine sulfate labeling of cells: implications for cellular magnetic resonance imaging. NMR Biomed.